# Cy5.5-Aminohexanoic acid-RPLALWRS-aminohexanoic acid-C-G4-PAMAM-PEG-AF750

Chemical name: | Cy5.5-Aminohexanoic acid-RPLALWRS-aminohexanoic acid-C-G4-PAMAM-PEG-AF750
Abbreviated name: | PB-M7NIR
Synonym:
Agent category: | Peptide
Target: | Matrix metalloproteinase-7 (MMP-7)
Target category: | Enzyme
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal/contrast: | Cy5.5
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PB-M7NIR)]

Optical fluorescence imaging is increasingly used to obtain biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging.

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (3). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (4). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (5).

Several families of MMPs are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastases (6-9). MMP expression in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages, is highly regulated. Elevated levels of MMPs have been found in tumors associated with a poor prognosis for cancer patients (10). The peptide aminohexanoic acid(AXH)-RPLALWRS-(AXH)-C (M7) was found to be a MMP-7 substrate that is cleaved between the L and W residues. Scherer et al. (11) used this sequence with a Cy5.5 NIR dye molecule to attach to a Generation 4–polyamidoamine-polyethylene glycol (PEG)-AF750 dendrimer to form fluorescence-quenched dendrimer, Cy5.5-(AXH)-RPLALWRS-(AXH)-C-G4-PAMAM-PEG-AF750 (PB-M7NIR). The Cy5.5 molecules are in close proximity, which results in fluorescence quenching because of the close proximity of the Cy5.5 molecules. AF750 molecules are conjugated to the dendrimer and act as an internal fluorescence reference. The NIR fluorescence signal will increase when the L-W bond is cleaved by MMP-7, releasing Cy5.5-containing fragments. Cy5.5 is a NIR fluorescent dye with an absorbance maximum at 675 nm and an emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^. PB-M7NIR is being developed for NIR fluorescence imaging of MMP-7 expression in tumors, atherosclerosis, myocardial infarction, and other diseases.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PB-M7NIR%20and%20synthesis)]

Scherer et al. (11) prepared PB-M7NIR by conjugation of Cy5.5-M7 to G4-PAMAM-PEG-AF750. A methanolic solution (5 mM) of the M7 peptide was reacted with 0.8 molar equivalent of Cy5.5-NHS in dimethyl sulfoxide (DMSO) (7 mM), and triethylamine was added to 1% (v/v) to fluorescently label the peptide at the N-terminal amine. Cy5.5-M7 was coupled to G4-PAMAM-PEG. To synthesize the thioether-bonded conjugate in Cy5.5-M7-PAMAM-PEG, the PAMAM-PEG conjugate was first activated by treatment with N-succinimidyl iodoacetate (SIA) (8 mg/ml methanol, 20 molar equivalents/PAMAM). After reaction for 20 minutes at room temperature, the SIA-activated PAMAM-PEG was incubated with the reduced Cy5.5-M7 peptides in methanolic solution (8 peptides/PAMAM) for 24 hours at room temperature. To label the PAMAM dendrimer scaffold with AF750, the Cy5.5-M7-PAMAM-PEG was dissolved in 50 mM in Na_2_CO_3_ (pH 9) and reacted for 18 h with up to 8 molar equivalents of AF750-NHS (7 mM in DMSO). PB-M7NIR was purified with ultrafiltration. There were approximately eight molecules of Cy5.5-M7 and approximately six molecules of AF750 per PB-M7NIR.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PB-M7NIR%20and%20in%20vitro)]

Scherer et al. (11) showed that PB-M7NIR exhibited five-fold increases in Cy5.5 NIR fluorescence signal with MMP-7 incubation with no change in the AF750 reference fluorescence signal. McIntyre et al. (12) showed that FITC-M7-PAMAM-TMR (PB-M7VIS) was cleaved by MMP-2, MMP-3, and MMP-7. However, PB-M7VIS was 56-fold more active with MMP-7 than with MMP-2 and 13-fold more active with MMP-7 than with MMP-3. PB-M7VIS was not a substrate for cathepsin B or L.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PB-M7NIR%20and%20rodentia)]

Scherer et al. (11) performed biodistribution studies of PB-M7NIR (1 nmol/mouse) injected intravenously to mice (n = 13) bearing SW480neo human colon cancer cells (MMP-7–negative) on one flank and SW480mat human colon cancer cells (MMP-7–positive) on the opposite flank. Optical imaging was performed in the Cy5.5 and AF750 channels for 4 h after injection. Cy5.5 NIR fluorescence signal above the background was visualized at 1 h and increased by approximately one-fold at 3 h as compared with the signal at 1 h. On the other hand, the AF750 reference signal was lower than the Cy5.5 signal with little increase over time. The Cy5.5/AF750 ratios at 4 h after injection were 70 for the MMP-7–negative tumors and 275 for the MMP-7–positive tumors. Histological imaging of tumor sections revealed a strong Cy5.5 signal at the tumor-stroma interface and in the ECM of MMP-7–positive tumor sections, but not in the MMP-7–negative tumor sections with Cy5.5/AF750 ratios of 692 and 2, respectively. No blocking or MMP-7 inhibition experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PB-M7NIR%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PB-M7NIR%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PB-M7NIR%20and%20human)]

No publication is currently available.

## NIH Support

R01 CA60867, P30 068485

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
4 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
5 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
6 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
7 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
8 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
9 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
10 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
11 Scherer R.L., VanSaun M.N., McIntyre J.O., Matrisian L.M. (2008). Optical imaging of matrix metalloproteinase-7 activity in vivo using a proteolytic nanobeacon. Mol Imaging.
12 McIntyre J.O., Fingleton B., Wells K.S., Piston D.W., Lynch C.C., Gautam S., Matrisian L.M. (2004). Development of a novel fluorogenic proteolytic beacon for in vivo detection and imaging of tumour-associated matrix metalloproteinase-7 activity. Biochem J.